# ^64^Cu-Labeled Lys^40^(1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid)NH_2_–conjugated exendin-4

Chemical name: | ^64^Cu-Labeled Lys^40^(1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid)NH_2_–conjugated exendin-4
Abbreviated name: | [^64^Cu](Lys^40^(DOTA)NH_2_)Exendin-4
Synonym:
Agent Category: | Peptide
Target: | Glucagon-like peptide 1 receptor (GLP-1R)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Exendin%204)]

Autoimmune processes and other environmental factors that destroy β-cells located in the pancreatic islet cells are known to promote the development of insulin-dependent diabetes mellitus (type 1 diabetes) in individuals genetically predisposed to the disease (1). Due to this destruction, the net mass of the β-cells in the islet cells of the pancreas is reduced, which leads to decreased production of insulin in the individual, and the maintenance of blood glucose at proper physiological levels is impaired. Type 2 diabetes is the most common form of the disease and is primarily caused by insulin resistance as a consequence of low insulin secretion by the β-cells. This form of diabetes can often be corrected with exercise, diet control, and/or medication (2). Upon diagnosis of diabetes, it is important to determine the individual's β-cell mass (BCM) or volume to devise a successful treatment regimen for the condition (3). Changes in the BCM during the onset of diabetes is poorly understood, and only an indirect method that measures the amount of stimulated insulin secretion by the pancreas is used to quantify the BCM in humans (4). However, the β-cells appear to have a reserved capacity to produce insulin, so the use of insulin secretion as a determinant of BCM is of limited value (4).

As an alternative to determine insulin secretion to quantify BCM, investigators have evaluated the use of noninvasive positron emission tomography (PET) imaging techniques to determine the BCM in rats with the use of ^11^C- or ^18^F-labeled dihydrotetrabenazine, which is an antagonist of the vesicular monoamine transporter type 2 (VMAT2) in the islet cells (5). Careful evaluation of results obtained with the VMAT2 antagonists has revealed that a large proportion of these radiolabeled compounds tend to reside in the exocrine pancreas, indicating that these radiotracers are not suitable for the determination of BCM with PET imaging (6). Recently, some G-protein–coupled receptors (e.g., the glucagon-like peptide 1 (GLP 1) receptor (GLP-1R)), which show a selective location in the β-cells compared to the surrounding exocrine pancreatic cells, were identified by database mining and immunohistochemical staining of pancreatic tissue (6-8). On the basis of these observations and the known involvement of GLP-1R in β-cell function and biology (for details, see Baggio and Drucker (9)), this receptor was identified as a possible target of radiolabeled probes that can be used to quantify the BCM. Although GLP-1 is the natural ligand for the GLP-1R, a major drawback of using this peptide to measure the BCM is that it is rapidly inactivated (half-life, ~2 min) by proteolytic enzymes while in circulation. As a consequence, investigators identified and have used radiolabeled Exendin-4 or its analogs (Exendin is a peptide of 39 amino acids that has a 54% homology with GLP-1, acts as an agonist of the GLP-1R, and is not inactivated by proteolytic enzymes) for the measurement of BCM with noninvasive molecular imaging techniques (6, 8). Connolly et al. evaluated the use of ^64^Cu-labeled Lys^40^(1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid)NH_2_–conjugated exendin-4 ([^64^Cu](Lys^40^(DOTA)NH_2_)Exendin-4) for the in vivo imaging and measurement of the BCM in rats and investigated its biodistribution in these animals (6).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?term=BCM%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D&cmd=DetailsSearch)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=GLP-1R) related to GLP-1R

Gene information (http://www.ncbi.nlm.nih.gov/gene/2740) regarding human GLP-1R (Gene ID: 2740)

Glucagon-like peptide 1 (http://omim.org/entry/138030) in Online Mendelian Inheritance in Man Database (OMIM)

Mouse GLP-1R (http://www.genome.jp/dbget-bin/www_bget?mmu:14652) in Kyoto Encyclopedia of Genes and Genomes Database (KEGG)

GLP-1R agonists for the treatment of type II diabetes: Exenatide (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=751747da-7c1f-41ad-b1a6-a6d920f70599) and Liraglutide (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=5a9ef4ea-c76a-4d34-a604-27c5b505f5a4)

American Diabetes Association (http://www.diabetes.org/)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B(64)Cu%5D%20(Lys(40)(DOTA)NH(2))Exendin-4%20synthesis)]

(Lys^40^(DOTA)NH_2_)Exendin-4 was obtained from a commercial source and labeled with ^64^Cu as described by Connolly et al. (6). The labeled peptide was purified on a C_18_ light SepPak column with high-performance liquid chromatography. The radiochemical purity of the labeled peptide was determined to be 94.2 ± 0.9% with a specific activity of 13.22 ± 6.62 TBq/mmol (357 ± 179 Ci/mmol; n = 5 experiments). The stability of [^64^Cu](Lys^40^(DOTA)NH_2_)Exendin-4 was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B%2864%29Cu%5D%20%28Lys%2840%29%28DOTA%29NH%282%29%29Exendin-4%20in%20vitro&cmd=DetailsSearch)]

A commercially available kit that quantifies the amount of cyclic AMP produced by the activation of a receptor was used with Chinese hamster ovary cells that express the human GLP-1R to determine the agonistic potency of (Lys^40^(DOTA)NH_2_)Exendin-4 (used as a proof of concept molecule for the study) (6). The EC_50_ of this molecule was determined to be 0.41 nM; however, the EC_50_ values of GLP-1 and Exendin-4 were not reported.

In another study, normal and diabetic human and non-human primate pancreas sections were subjected to immunohistochemical analysis with appropriate antibodies to detect the presence of the GLP-1R in the organ (6). The fluorescent signal was detected only in islet cells of the normal specimens, and sections obtained from the diabetic organ generated a very low signal in these cells. This indicated that there was a low level of the GLP-1R in the diabetic specimens and suggested that the receptor could be a suitable target for the noninvasive imaging of β-cells.

Ex vivo autoradiography of pancreas sections obtained from a rat at 60 min after tail vein injection of [^64^Cu](Lys^40^(DOTA)NH_2_)Exendin-4 showed a distinct signal pattern in multiple areas of the tissue, and this was presumed to be generated by radioactivity bound to the islet cells (6). The same section was immunostained to detect insulin (insulin is stained only where the β-cells are present), and a staining pattern similar to that observed with [^64^Cu](Lys^40^(DOTA)NH_2_)Exendin-4 was apparent. The two images were merged, and the autoradiographic and the immunostaining signals were reported to originate from the same location in the specimen, indicating that the distribution of radioactivity corresponded to the distribution of the islet cells. Autoradiography of pancreas sections obtained from a rat administered with unlabeled Exendin(9-39) 10 min before the injection of [^64^Cu](Lys^40^(DOTA)NH_2_)Exendin-4 showed a complete absence of signal, suggesting that the uptake of radioactivity was blocked in this specimen and that the radiolabeled peptide had binding specificity for the GLP-1R. It was also reported that autoradiography of pancreas sections from Zucker ZDF rats (http://www.criver.com/en-us/prodserv/bytype/resmodover/resmod/pages/zdfrat.aspx) (these rodents are the animal model for human type 2 diabetes and show loss of β-cells with progression of the disease) injected with [^64^Cu](Lys^40^(DOTA)NH_2_)Exendin-4 showed very little uptake of radioactivity compared with pancreas sections obtained from control Zucker ZCL rat (6). These results indicated that the tracer was suitable for the determination of any changes in the BCM of the animals.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B(64)Cu%5D%20(Lys(40)(DOTA)NH(2))Exendin-4%20rodentia)]

The biodistribution of [^64^Cu](Lys^40^(DOTA)NH_2_)Exendin-4 was studied in normal and streptozotocine (http://www.sigmaaldrich.com/catalog/ProductDetail.do?D7=0&N5=SEARCH_CONCAT_PNO%7CBRAND_KEY&N4=85882%7CFLUKA&N25=0&QS=ON&F=SPEC) (STZ)-treated Sprague-Dawley rats (n = 3 animals/group) (6). Immediately prior to initiation of the study, the blood glucose levels of animals from both groups were determined. The rodents were injected with 1.1 MBq (30 μCi) of the tracer through the tail vein and euthanized 60 min later to determine the amount of radioactivity accumulated in the organs of interest. Data were reported as standard uptake values (SUV) corresponding to the injected dose and weight of each animal. The blood glucose level of the normal animals was significantly lower (98.0 ± 12.2 mg/dL; P = 0.02) than that of the STZ-treated rats (442.3 ± 42.7 mg/dL), indicating that the latter group of rodents had a complete onset of diabetes. Both groups of rats showed high accumulation of radioactivity in the kidneys (48.3 ± 5.5 SUV and 27.6 ± 5.1 SUV for the control and STZ-treated animals, respectively), indicating that the tracer was excreted primarily through the urinary system. Uptake of radioactivity in the pancreas of the STZ-treated animals (0.1 ± 0.01 SUV) was significantly lower (P = 0.001) than that observed in the organ of the control rats (0.3 ± 0.02 SUV). All other organs obtained from the control animals showed uptake values between 0.03 ± 0.02 SUV (blood) and 0.7 ± 0.2 SUV (liver), and the STZ-treated group showed a similar trend with tracer accumulation values between 0.2 ± 0.04 SUV (blood) and 0.6 ± 0.05 SUV (liver).

To confirm the uptake of [^64^Cu](Lys^40^(DOTA)NH_2_)Exendin-4 in the pancreas of the rats, dynamic PET images were acquired from two anesthetized animals (6). The rodents were first injected with [^11^C]methionine to visualize the pancreatic region in the abdomen of the animals (this tracer is known to accumulate primarily in the pancreas (6)). PET scans were performed for 45 min, and images obtained with the ^11^C probe clearly showed the outline of the pancreas of the animals. Subsequently, the same animals were injected with [^64^Cu](Lys^40^(DOTA)NH_2_)Exendin-4, and PET scans were acquired for 60 min post injection. To confirm the accumulation of the Exendin tracer in the pancreas, images obtained from the two separate scans were merged using appropriate software as described by Connolly et al. (6). In the merged image, however, the radioactivity taken up by the kidneys from the ^64^Cu-labeled peptide interfered with the image of the pancreas due to the close proximity of the organs in the abdominal cavity of the rats. As a result, the investigators could not clearly visualize the uptake of label in the pancreas.

From these studies, the investigators concluded that [^64^Cu](Lys^40^(DOTA)NH_2_)Exendin-4 bound specifically to the GLP-1R under in vitro conditions. To confirm this observation in vivo and to quantify the BCM in the pancreas, however, similar studies will have to be performed in large animals (6).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B%2864%29Cu%5D%20%28Lys%2840%29%28DOTA%29NH%282%29%29Exendin-4%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B%2864%29Cu%5D%20%28Lys%2840%29%28DOTA%29NH%282%29%29Exendin-4%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=17138746%5Buid%5D&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Concannon P., Rich S.S., Nepom G.T. (2009). Genetics of type 1A diabetes. N Engl J Med.
2 Krentz A.J., Bailey C.J. (2005). Oral antidiabetic agents: current role in type 2 diabetes mellitus. Drugs.
3 Ritzel R.A. (2009). Therapeutic approaches based on beta-cell mass preservation and/or regeneration. Front Biosci.
4 Harris P.E., Ferrara C., Barba P., Polito T., Freeby M., Maffei A. (2008). VMAT2 gene expression and function as it applies to imaging beta-cell mass. J Mol Med (Berl).
5 Kung M.P., Hou C., Lieberman B.P., Oya S., Ponde D.E., Blankemeyer E., Skovronsky D., Kilbourn M.R., Kung H.F. (2008). In vivo imaging of beta-cell mass in rats using 18F-FP-(+)-DTBZ: a potential PET ligand for studying diabetes mellitus. J Nucl Med.
6 Connolly B.M., Vanko A., McQuade P., Guenther I., Meng X., Rubins D., Waterhouse R., Hargreaves R., Sur C., Hostetler E. (2012). Ex Vivo Imaging of Pancreatic Beta Cells using a Radiolabeled GLP-1 Receptor Agonist. Mol Imaging Biol.
7 Cline G.W., Zhao X., Jakowski A.B., Soeller W.C., Treadway J.L. (2011). Islet-selectivity of G-protein coupled receptor ligands evaluated for PET imaging of pancreatic beta-cell mass. Biochem Biophys Res Commun.
8 Wang Y., Lim K., Normandin M., Zhao X., Cline G.W., Ding Y.S. (2011). Synthesis and evaluation of [(18)F]exendin (9-39) as a potential biomarker to measure pancreatic beta-cell mass. Nucl Med Biol.
9 Baggio L.L., Drucker D.J. (2007). Biology of incretins: GLP-1 and GIP. Gastroenterology.